# N-(4-[^18^F]Fluoro-benzoyl)-N'-{2-[5-(4-fluoro-benzyl)-1-(4-methoxy-benzyl)-4,6-dioxo-1,4,5,6-tetrahydro-[1,3,5]triazin-2-ylamino]-ethyl}-guanidine

Chemical name: | N-(4-[^18^F]Fluorobenzoyl)-N'-{2-[5-(4-fluoro-benzyl)-1-(4-methoxy-benzyl)-4,6-dioxo-1,4,5,6-tetrahydro-[1,3,5]triazin-2-ylamino]-ethyl}-guanidine
Abbreviated name: | [^18^F]PC-10
Synonym:
Agent category: | Compound
Target: | Prokineticin receptor 1 (PKR1, PROKR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=prokineticin%20receptor)]

Bv8 is a small protein secreted by frog skin (1). The prokineticins PK1 and PK2, which are mammalian homologs of Bv8, and their G-protein–coupled receptors prokineticin receptor 1 (PKR1) and prokineticin receptor 2 (PKR2) have been identified and linked to several biological functions such as gut motility, neurogenesis, angiogenesis, circadian rhythms, hematopoiesis, and nociception (2-4). Prokineticins are also associated with pathologies of the reproductive and nervous systems, myocardial infarction, and tumorigenesis. PKR1 shares 33% identity with human neuropeptide Y receptor-2, and PKR1 is expressed in the brain, spleen, prostate, testis, leukocytes, pancreas, adrenal gland, thyroid, salivary gland, pituitary, stomach, small intestine, colon, and rectum. On the other hand, PKR2 is expressed mainly in the ileocecum and discrete nuclei of the central nervous system. PK1 is secreted by endocrine glands, whereas PK2 is highly expressed in the bone marrow, lymphoid organs, and leukocytes, which suggests a role for PK2 in inflammation, immunomodulation, and hematopoiesis. Binding of PK2 to PKR1 has been shown to reduce the pain threshold in sensory neurons and can contribute to inflammatory pain. PK2 is highly expressed by neutrophils and other inflammatory cells as a pronociceptive mediator in inflamed tissues.

Several nonpeptidic PK antagonists have been developed for pain reduction and cancer therapy (5). However, noninvasive quantification of PKR1 levels in vivo is not available for drug development. A nonpeptidic PKR1 antagonist, N-{2-[5-(4-fluoro-benzyl)-1-(4-methoxy-benzyl)-4,6-dioxo-1,4,5,6-tetrahydro-[1,3,5]triazin-2-ylamino]-ethyl}-guanidine (PC-7), which contains a free guanidine group, was labeled with ^18^F by reacting the guanidine moiety with N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]FBA) to form N-(4-[^18^F]fluoro-benzoyl)-N'-{2-[5-(4-fluoro-benzyl)-1-(4-methoxy-benzyl)-4,6-dioxo-1,4,5,6-tetrahydro-[1,3,5]triazin-2-ylamino]-ethyl}-guanidine ([^18^F]PC-10). Jacobson et al. (6) evaluated [^18^F]PC-10 binding in mice injected with complete Freund adjuvant (CFA) to induce inflammatory pain by upregulation of PK2 and PKR1.

### Related Resource Links:

- Chapters in MICAD (Prokineticin receptor 1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Prokineticin%20receptor%201%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Prokineticin receptor 1 (http://www.ncbi.nlm.nih.gov/gene/10887), prokineticin 1 (http://www.ncbi.nlm.nih.gov/gene/84432))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Prokineticin receptor 1 (http://www.ncbi.nlm.nih.gov/omim/607122), prokineticin 1 (http://www.ncbi.nlm.nih.gov/omim/606233))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PC-10%20and%20synthesis)]

Jacobson et al. (6) prepared [^18^F]PC-10 with a two-step synthesis in a modular system. [^18^F]FBA was synthesized using a standard nucleophilic radiofluorination ([^18^F]KF/Kryptofix 2.2.2) reaction, with 50%–60% yield and >99% radiochemical purity. [^18^F]FBA and PC-7 were incubated in dimethylformamide for 10 min at 60°C. [^18^F]PC-10 was purified with high-performance liquid chromatography, with a radiochemical purity of >99% and a specific activity of 70.2 ± 7.4 GBq/µmol (1.9 ± 0.2 Ci/µmol) at the end of synthesis. The overall decay-corrected yield was 16 ± 3% (n = 4). The total synthesis time was ~160 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PC-10%20and%20in%20vitro)]

Chinese hamster ovary (CHO) cells were transfected with human PKR1 or human PKR2 (6). A receptor-binding assay was performed with ^125^I-Mamba intestinal toxin-1, a Bv8 homolog. [^18^F]PC-10 exhibited 50% inhibition concentration (IC_50_) values of 109.7 ± 4.9 nM and 1,200 ± 69 nM for PKR1 and PKR2, respectively. [^18^F]PC-10 accumulated rapidly in CHO-PKR1 cells with 30 min of incubation at 37°C, and ~50% of radioactivity was internalized with up to 2 h of incubation. Retention studies showed a rapid release of radioactivity by CHO-PKR1 cells in fresh medium; 50% of radioactivity was unbound at 15 min, and radioactivity levels reached a plateau after 1 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PC-10%20and%20rodentia)]

Jacobson et al. (6) performed static positron emission tomography scans in a CFA-induced inflammatory pain model in mice (n = 3–5/group) at 0.5, 1, and 2 h after injection of 1.85 MBq (0.05 mCi) [^18^F]PC-10. Accumulation of [^18^F]PC-10 in the inflamed paws was determined to be 0.95 ± 0.20% injected dose/gram (ID/g), 1.21 ± 0.32% ID/g, and 0.78 ± 0.04% ID/g at 0.5, 1, and 2 h, respectively. Accumulation in the control paws was 0.13–0.25% ID/g at these time points. [^18^F]PC-10 accumulation in the inflamed paws was significantly higher than in the control paws at these three time points (P < 0.01), with inflamed paw/control paw ratios of 4.2–5.7. In comparison, 2-[^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/pubmed/20641537)) provided inflamed paw/control paw ratios of ~2 at these time points. [^18^F]PC-10 accumulation was high in the PKR1-expressing organs, such as the gastrointestinal tract (54.3% ID/g) and salivary gland (3.05% ID/g), at 2 h after injection. The liver (3.80% ID/g) and kidneys (5.26% ID/g) exhibited moderate accumulation, and blood (0.22% ID/g) and bone (0.69% ID/g) had low radioactivity levels. Coinjection with excess PC-7 (0.3 mg) reduced the radioactivity level in the inflamed paws by 70% at 1 h after injection. Effect of PC-7 on [^18^F]PC-10 accumulation in other tissues was not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PC-10%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PC-10%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PC-10%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Negri L., Lattanzi R., Giannini E., Canestrelli M., Nicotra A., Melchiorri P. (2009). Bv8/Prokineticins and their Receptors A New Pronociceptive System. Int Rev Neurobiol.
2 Lin D.C., Bullock C.M., Ehlert F.J., Chen J.L., Tian H., Zhou Q.Y. (2002). Identification and molecular characterization of two closely related G protein-coupled receptors activated by prokineticins/endocrine gland vascular endothelial growth factor. J Biol Chem.
3 Podlovni H., Ovadia O., Kisliouk T., Klipper E., Zhou Q.Y., Friedman A., Alfaidy N., Meidan R. (2006). Differential expression of prokineticin receptors by endothelial cells derived from different vascular beds: a physiological basis for distinct endothelial function. Cell Physiol Biochem.
4 Zhou Q.Y. (2006). The prokineticins: a novel pair of regulatory peptides. Mol Interv.
5 Balboni G., Lazzari I., Trapella C., Negri L., Lattanzi R., Giannini E., Nicotra A., Melchiorri P., Visentin S., Nuccio C.D., Salvadori S. (2008). Triazine compounds as antagonists at Bv8-prokineticin receptors. J Med Chem.
6 Jacobson O., Weiss I.D., Niu G., Balboni G., Congiu C., Onnis V., Kiesewetter D.O., Lattanzi R., Salvadori S., Chen X. (2011). Prokineticin receptor 1 antagonist PC-10 as a biomarker for imaging inflammatory pain. J Nucl Med.